# 2-((2-((Dimethylamino)methyl)phenyl)thio)-5-[^123^I]iodophenylamine

Chemical name: | 2-((2-((Dimethylamino)methyl)phenyl)thio)-5-[^123^I]iodophenylamine
Abbreviated name: | Radioiodinated ADAM
Synonym: | 2-[2-(dimethylaminomethyl)phenyl]sulfanyl-5-iodoaniline
Agent Category: | Compound
Target: | Serotonin transporter (SERT)
Target Category: | Binding to SERT
Method of detection: | SPECT, planar scintigraphy
Source of signal: | ^123^I/^125^I
Activation: | Not required
Studies: | - In vitro; - Rodents; - Non-primate non-rodent mammals; - Non-human primates; - Humans | Click on the above structure for additional information in PubChem (http://pubchem.ncbi.nlm.nih.gov).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+ADAM)]

Serotonin (5-HT) is now known to serve as the gastrointestinal signaling molecule and participate in the development of alcohol dependence (1, 2). It is also involved in a variety of physiological functions such as the post-meal satiety process, as well as the pathogenesis of Alzheimer’s and Parkinson’s diseases, anxiety, and depression (1-3). Imaging and data obtained by the analysis of resected tissue of epileptic patients and studies in animal models have provided much evidence that endogenous 5-HT, the activity of its receptors, and pharmaceuticals with 5-HT agonist and/or antagonist activities are believed to be involved in the pathogenesis of epilepsy (4). Thus, imaging of the 5-HT system (SERT) is considered important to understand a variety of neurological and psychiatric functions and disorders.

A variety of drugs have been labeled with radioactive iodine (^123^I), carbon (^11^C), or fluorine (^18^F) for imaging of the 5-HT receptor or transporter using positron emission tomography (PET) or single-photon emission computed tomography (SPECT) (5). In general, these compounds are either nonselective or have a low specificity for SERT (6). Subsequently, a new drug, 2-((2-((dimethylamino)methyl)phenyl)thio)-5-iodophenylamine (ADAM), radioiodinated with ^123^I or ^125^I, has been evaluated by several investigators for imaging of SERT.

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+ADAM+synthesis)]

The synthesis of ADAM has been detailed by Oya et al. (7). A mixture of 2,5-dibromonitrobenzene, 2-thio-N,N,-dimethylbenzamide, and potassium carbonate in dimethylformamide was heated at 100°C for 24 h. The mixture was added to cold water, and the precipitates were collected and recrystalized from ethanol. This reaction produced a light yellow solid, 2-(4-bromo-2-nitrophenylthio)-N,N-dimethylbenzamide, with a yield of 79%. The light yellow solid was dissolved in tetrahydrofuran (THF), and a mixture of borane (BH_3_) in THF was added to it. The mixture was refluxed for 2 h and stirred overnight at room temperature. The solvent was removed under reduced pressure to obtain a residue. Water was added to the residue, and the mixture was refluxed for 30 min with vigorous stirring. The solution was neutralized (pH 7–8) with sodium bicarbonate and extracted three times with a mixture of dichloromethane and methanol. The extractions were combined and dried over sodium sulphate, and the solvent was removed under reduced pressure. The residue was purified by silica gel chromatography, and a colorless oil, 2-(4-bromo-2-nitrophenylthio)-benzyl)dimethylbenzamide, with a yield of 83%, was obtained.

The nitro group was reduced in a mixture of HCl, methanol, and stannous chloride at 10°C. With this reaction a residue of 5-bromo-2-((2-((diethylamino)methyl)phenyl)thio)phenylamine was obtained with a yield of 78%. This residue was dissolved in triethylamine, and bis(tributyltin) and tetrakis(triphenylphosphine)palladium were added to it. The mixture was heated to 100°C in a sealed bottle for 48 h, and the solvent was subsequently removed under reduced pressure. A residue of 2-((2-((dimethylamino)methyl)phenyl)thio)-5-(tri-n-butyltin)-phenylamine was obtained as a colorless oil and purified on preparative silica gel plates. The yield of this reaction was 59%.

The colorless oil was dissolved in chloroform, and a solution of iodine in chloroform was added drop-wise until the iodine color persisted. The solution was stirred overnight at room temperature, and a solution of potassium fluoride in methanol was added. A solution of sodium bisulphate was added to the mixture and stirred for 5 min. The organic layer was separated and dried over sodium sulphate, and the solvent was removed under reduced pressure. The final product, ADAM, which is a colorless oil, was purified on preparative silica gel plates. This reaction had a yield of 99%.

To prepare radioiodinated ADAM, ^123^I/^125^I-labeled sodium iodide in 1 N HCl was mixed with 2-((2-((dimethylamino)methyl)phenyl)thio)-5-(tri-n-butyltin)-phenylamine in a sealed vial, and hydrogen peroxide was added through a syringe at room temperature. The iodination reaction was terminated after 10 min by the addition of saturated sodium persulphate, and the resulting solution was neutralized with sodium bicarbonate solution. The mixture was extracted with ethyl acetate, and the organic layer (purity, 90%; yield, 94%) was dried over sodium sulphate. The solvent was then removed under a stream of dry nitrogen, and the residue was purified by high-performance liquid chromatography. The radiochemical purity of the product was 99%. The specific activities of the compounds were not reported by the investigators, although the stability of [^125^I]ADAM was reported to be 3 months under refrigerated conditions. The corresponding [^123^I]ADAM was reported to be stable for 24 h after labeling. Another group of investigators who prepared [^123^I/^125^I]ADAM by a similar method reported the specific activity to be 8.88 × 10^6^ GBq/mmol (240,000 Ci/mmol) for [^123^I]ADAM and 8.14 × 10^4^ GBq/mmol (2,200 Ci/mmol) for [^125^I]ADAM (8).

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+ADAM+in+vitro)]

Using rat frontal cortical membrane homogenates for saturation binding studies with [^125^I]ADAM, the radiochemical had a dissociation constant (K_d_) of 0.15 ± 0.03 nM and a B_max_ of 194 ± 65 fmol/mg protein (8). In another study, the binding affinity (K_i_) of [^125^I]ADAM toward SERT on cloned LLC-PK1 cell membranes (of pig kidney origin) was 0.013 nM with a >1,000 fold selectivity over the respective norepinephrine (K_i_ = 699 nM) and dopamine (K_i_ = 840 nM) transporters.

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+ADAM+rodents)]

Oya et al. observed 60–240 min after administration of [^125^I]ADAM that the rat brain showed an excellent label uptake (1.4% of the total dose at 2 min) consistently located in the hypothalamus, the organ with the highest concentration of SERT in the body (7). Choi et al. showed that the hypothalamic uptake of [^125^I]ADAM in rats was blocked by pretreatment with SERT-selective competing drugs such as paroxetine and (+)McN5652 (8).

The biodistribution of [^123^I]ADAM in mice and in individual organs and tissue was studied with whole-body autoradiography (WBAR) (9). The liver was found to have the highest uptake. By WBAR it was demonstrated that the label bound to SERT-rich sites found in the brain stem, lungs, adrenal glands, and the intestinal mucosa. The investigators concluded that radioiodinated ADAM was a suitable agent for the investigation and imaging of SERT in the central and peripheral nervous system, as well as the neuroendocrine tissue. From another study on rats and mice in the same laboratory, it was concluded that [^123^I]ADAM accumulates in the same SERT-rich areas of the brain in both rats and mice (10). Uptake of the label in SERT-rich areas of the brain was inhibited by treatment with p-chloroamphetamine, a potent neurotoxin that causes the release and depletion of 5-HT in the central nervous system. The investigators concluded that [^123^I]ADAM was an appropriate radioligand to study SERT function in humans. With a similar study in rats, Chalon et al. also concluded that [^125^I]ADAM could be used to investigate central 5-HT system dysfunction in humans (11).

In another study, Hwang et al. concluded that SERT availability could be assessed semi-quantitatively in small animals by SPECT with radioiodinated ADAM (12).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+ADAM+Non-Primate+Mammals)]

Ye et al. investigated the biodistribution of [^123^I]ADAM in the rabbit brain by SPECT. Maximum label was observed to accumulate in the brain stem 90–120 min after injection with a target/background ratio of 1.89 ± 0.02 (13). The investigators concluded that [^123^I]ADAM was a suitable selective agent to investigate SERTs with SPECT.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+ADAM+non-human+primate+studies)]

A preliminary SPECT imaging study of [^123^I]ADAM was conducted in baboons (7). A specific uptake of the label in the midbrain region, with a high concentration of SERT, of the animals was observed 180–240 min after administration of the radiopharmaceutical.

In another study from the same laboratory, the investigators used [^123^I]ADAM and SPECT imaging to quantify SERT in baboon brains (Papio anubis) (14). Acton et al. used dynamic imaging and metabolite-corrected plasma data to determine the distribution volume (DV) of different regions of the brain and the distribution volume ratio (DVR) of target to cerebellum (CB); the CB was used as the reference tissue because it contains the lowest concentration of SERT compared to other parts of the brain). The mean DVs in the midbrain (MB) and CB were 4.86 ± 1.06 mL/mL and 2.25 ± 0.48 mL/mL, respectively. The MB DVR was 2.01 ± 0.17. From this study the investigators concluded that dynamic modeling of [^123^I]ADAM SPECT scans could be used accurately and reproducibly to quantify SERT in non-human primates.

Huang et al. used SPECT with [^123^I]ADAM in monkeys (Macaca cyclopis) to study the imaging of SERT (15). Using CB as the reference tissue, the investigators determined the specific uptake ratios (SURs) of the MB, thalamus (TH), striatum (ST), temporal and frontal cortices, and the whole brain. The SURs were ~3, ~2, and ~1 for the MB, TH, and ST, respectively, and the ratio was <1 for other regions of the brain. The SURs reached equilibrium in the MB, TH, and ST ~210 min after injection.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/sites/entrez?Db=pubmed&Cmd=DetailsSearch&Term=123I+ADAM+human+)]

SPECT was used in two laboratories to investigate the biodistribution of [^123^I]ADAM in humans (6, 16). An analysis of the combined data from the two studies revealed that the radiolabel accumulated in the MB with a distribution that was consistent with selective binding to SERT (16). The region/CB ratios for the SPECT scans were 1.95 ± 0.13 for the MB, 1.27 ± 0.10 for the medial temporal regions, and 1.11 ± 0.07 for the ST. The investigators concluded that [^123^I]ADAM was a safe and suitable radiochemical for SERT imaging in the human brain. In a preliminary study, the binding of [^123^I]ADAM was investigated in human patients with major depressive disorder and normal healthy controls (17). Results from this study suggested that, compared to the control individuals, there was a decreased binding of the label in the MB region of the major depressive disorder patients that correlated with the severity of the depressive symptoms. The investigators also observed an age-related decrease in binding of the label in the MB SERT of the control subjects.

Using healthy volunteers, Booij and de Win as well as other investigators reported that the optimal imaging time for [^123^I]ADAM SPECT was ~5 h after a single injection of the radiochemical (18-20).

To determine the possible involvement of a SERT-related endophenotype for purging or non-purging bulimia nervosa (BN), the binding of [^123^I]ADAM was investigated in female twins (21). The purging BN women were observed to have a higher binding of the label in the MB compared to the non-purging BN women and the normal controls. The investigators concluded that, because this study was performed in a small group (13 BN patients), the results should be interpreted with caution and the observations should be verified with a study involving a larger population. In another study, it was shown there was a significant (P < 0.001) increase in brainstem SERT availability in individuals suffering from migraines (22). However, the investigators suggested that whether SERT played a direct or an indirect role in the development of this condition remains to be determined.

## References

1 Halford J.C., Harrold J.A., Boyland E.J., Lawton C.L., Blundell J.E. (2007). Serotonergic drugs : effects on appetite expression and use for the treatment of obesity. Drugs.
2 Schule C. (2007). Neuroendocrinological mechanisms of actions of antidepressant drugs. J Neuroendocrinol.
3 Suehiro M., Greenberg J.H., Shiue C.Y., Gonzalez C., Dembowski B., Reivich M. (1996). Radiosynthesis and biodistribution of the S-[18F]fluoroethyl analog of McN5652. Nucl Med Biol.
4 Bagdy G., Kecskemeti V., Riba P., Jakus R. (2007). Serotonin and epilepsy. J Neurochem.
5 Moresco R.M., Matarrese M., Fazio F. (2006). PET and SPET molecular imaging: focus on serotonin system. Curr Top Med Chem.
6 Kauppinen T.A., Bergstrom K.A., Heikman P., Hiltunen J., Ahonen A.K. (2003). Biodistribution and radiation dosimetry of [123I]ADAM in healthy human subjects: preliminary results. Eur J Nucl Med Mol Imaging.
7 Oya S., Choi S.R., Hou C., Mu M., Kung M.P., Acton P.D., Siciliano M., Kung H.F. (2000). 2-((2-((dimethylamino)methyl)phenyl)thio)-5-iodophenylamine (ADAM): an improved serotonin transporter ligand. Nucl Med Biol.
8 Choi S.R., Hou C., Oya S., Mu M., Kung M.P., Siciliano M., Acton P.D., Kung H.F. (2000). Selective in vitro and in vivo binding of [(125)I]ADAM to serotonin transporters in rat brain. Synapse.
9 Lin K.J., Ye X.X., Yen T.C., Wey S.P., Tzen K.Y., Ting G., Hwang J.J. (2002). Biodistribution study of [(123)I] ADAM in mice: correlation with whole body autoradiography. Nucl Med Biol.
10 Lin K.J., Yen T.C., Wey S.P., Hwang J.J., Ye X.X., Tzen K.Y., Fu Y.K., Chen J.C. (2004). Characterization of the binding sites for 123I-ADAM and the relationship to the serotonin transporter in rat and mouse brains using quantitative autoradiography. J Nucl Med.
11 Chalon S., Bronquard C., Vercouillie J., Kodas E., Garreau L., Bodard S., Emond P., Besnard J.C., Guilloteau D. (2004). ADAM is an effective tool for in vivo study of serotonergic function: validation in rat models. Synapse.
12 Hwang L.C., Chang C.J., Liu H.H., Kao H.C., Lee S.Y., Jan M.L., Chen C.C. (2007). Imaging the availability of serotonin transporter in rat brain with 123I-ADAM and small-animal SPECT. Nucl Med Commun.
13 Ye X.X., Hwang J.J., Hsieh J.F., Chen J.C., Chou Y.T., Tu K.Y., Wey S.P., Ting G. (2004). In vivo quantification by SPECT of [123I] ADAM bound to serotonin transporters in the brains of rabbits. Nucl Med Biol.
14 Acton P.D., Choi S.R., Hou C., Plossl K., Kung H.F. (2001). Quantification of serotonin transporters in nonhuman primates using [(123)I]ADAM and SPECT. J Nucl Med.
15 Huang W.S., Ma K.H., Cheng C.Y., Chen C.Y., Fu Y.K., Chou Y.H., Wey S.P., Liu J.C. (2004). Imaging serotonin transporters with 123I-ADAM brain SPECT in healthy non-human primates. Nucl Med Commun.
16 Newberg A.B., Plossl K., Mozley P.D., Stubbs J.B., Wintering N., Udeshi M., Alavi A., Kauppinen T., Kung H.F. (2004). Biodistribution and imaging with (123)I-ADAM: a serotonin transporter imaging agent. J Nucl Med.
17 Newberg A.B., Amsterdam J.D., Wintering N., Ploessl K., Swanson R.L., Shults J., Alavi A. (2005). 123I-ADAM binding to serotonin transporters in patients with major depression and healthy controls: a preliminary study. J Nucl Med.
18 Booij J., de Win M.M. (2006). Brain kinetics of the new selective serotonin transporter tracer [(123)I]ADAM in healthy young adults. Nucl Med Biol.
19 Catafau A.M., Perez V., Penengo M.M., Bullich S., Danus M., Puigdemont D., Pascual J.C., Corripio I., Llop J., Perich J., Alvarez E. (2005). SPECT of serotonin transporters using 123I-ADAM: optimal imaging time after bolus injection and long-term test-retest in healthy volunteers. J Nucl Med.
20 Sacher J., Asenbaum S., Klein N., Geiss-Granadia T., Mossaheb N., Poetzi C., Attarbaschi T., Lanzenberger R., Spindelegger C., Rabas A., Heinze G., Dudczak R., Kasper S., Tauscher J. (2007). Binding kinetics of 123I[ADAM] in healthy controls: a selective SERT radioligand. Int J Neuropsychopharmacol.
21 Koskela A.K., Keski-Rahkonen A., Sihvola E., Kauppinen T., Kaprio J., Ahonen A., Rissanen A. (2007). Serotonin transporter binding of [123I]ADAM in bulimic women, their healthy twin sisters, and healthy women: a SPET study. BMC Psychiatry.
22 Schuh-Hofer S., Richter M., Geworski L., Villringer A., Israel H., Wenzel R., Munz D.L., Arnold G. (2007). Increased serotonin transporter availability in the brainstem of migraineurs. J Neurol.